# 3-Cyano-4-[^18^F]fluoro-benzoyl-Ala(SO_3_H)-Ava-Gln-Trp-Ala-Val-NMeGly-His-Sta-Leu-NH_2_

Chemical name: | 3-Cyano-4-[^18^F]fluoro-benzoyl-Ala(SO_3_H)-Ava-Gln-Trp-Ala-Val-NMeGly-His-Sta-Leu-NH_2_ | [image]
Abbreviated name: | [^18^F]7b | [image]
Synonym: | | [image]
Agent Category: | Peptides | [image]
Target: | Gastrin-releasing peptide receptor (GRPR) | [image]
Target Category: | Receptors | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^18^F | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of [^18^F]7b

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=GRPR+and+bombesin+and+imaging)]

3-Cyano-4-[^18^F]fluoro-benzoyl-Ala(SO_3_H)-Ava-Gln-Trp-Ala-Val-NMeGly-His-Sta-Leu-NH_2_, abbreviated as [^18^F]7b, is a bombesin (BN)-based ^18^F-labeled peptide synthesized by Mu et al. for positron emission tomography (PET) of tumors expressing gastrin-releasing peptide receptor (GRPR) (1).

BN is an amphibian neuropeptide consisting of 14 amino acids (pGlu-Gln-Arg-Leu-Gly-Asn-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_) (2). The C-terminal region of BN is responsible for its receptor binding and signal transduction (3). BN and its mammalian counterpart, gastrin-releasing peptide (GRP), produce a wide range of biological responses in diverse tissues (3). They also act as growth factors for cancer cells. Of the BN receptors, GRPR (also known as BB_2_ or BRS2) is best characterized (2). GRPR is a glycosylated G-protein–coupled receptor and is normally expressed in non-neuroendocrine tissues of the breast and pancreas and in neuroendocrine cells of the brain, gastrointestinal tract, lung, and prostate (1). Because GRPR is overexpressed in various tumors, a large number of BN analogs have been tested for GRPR-targeted imaging and therapy (4, 5). These analogs have been synthesized on the basis of either truncated BN (6–14 or 7–14) or full-length BN (1–14), and most analogs exhibit a high affinity to GRPR (6, 7). The truncated BN analogs appear more stable in vivo than the full-length tetradecapeptides, but the full-length peptides offer more labeling options by attachment of functional groups to the amino acids on positions 1 to 6 (8-10). For most analogs, the amino acids on positions 13 (Leu) and 14 (Met) have been replaced with non-natural amino acids for increasing stability, and Lys has been placed on position 3 for attaching radiolabels. Spacers, chelators, or radiometals have also been widely used for conjugation and for favorable kinetics (1, 4, 9). Functionally, most BN analogs act as agonists, and only a few to date are antagonists (8, 11). Agonists are internalized into and accumulate within cells, and they have been assumed to exhibit higher uptake by cancer cells than antagonists. However, some studies have shown that tumor uptake of antagonists is higher than that of agonists because antagonists may have stronger binding for GRPR than agonists (11).

Mu et al. synthesized a series of BN-based peptides by using different linkers, peptide sequences, and non-natural amino acids (1, 12). These peptides have been labeled with ^18^F with a one-step approach via^18^F-for-^+^N(CH_3_)_3_ substitution using a less lipophilic benzonitrile labeling moiety. Amino acids such as His, Trp, Arg, and non-natural amino acids such as statine (Sta) and cysteine sulfonic acid (Ala(SO_3_H)) in the peptide sequence did not require any protection group during radiosynthesis. Two analogs, one named as [^18^F]6b and another [^18^F]7b, exhibited specific uptake in GRPR-expressing PC-3 tumors and the pancreas in nude mice (1). [^18^F]6b is positively charged, while [^18^F]7b is negatively charged. Compared to [^18^F]6b, [^18^F]7b exhibits superior tumor uptake, is higher in specificity, and has more favorable tumor/nontarget ratios (1). The data suggest that [^18^F]7b is a promising PET tracer candidate for the diagnosis of GRPR-positive tumors in humans. This chapter describes the data obtained with [^18^F]7b. The data obtained with [^18^F]6b are described in the MICAD chapter on [^18^F]6b (http://www.ncbi.nlm.nih.gov/books/NBK5330/).

### Related Resource Links:

- Protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=4885361), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=61677286) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2925) information for GRPR
- Structure information of BN and analogs in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance/?term=bombesin)
- GRPR-targeted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=GRPR%20AND%20micad%5bbook%5d)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20857927)]

Mu et al. synthesized [^18^F]7b on the basis of the amino acid sequence 7–14 of the natural BN (1). Met^14^ was replaced with Leu for stabilization against aminopeptidases, and Leu^13^ was replaced with Sta for prevention of neutral endopeptidase cleavage. Gly^11^ was changed to its methylated version (NMeGly). A polar spacer, Ala(SO_3_H)-Ava, was inserted between the labeling moiety and the binding sequence to improve the peptide pharmacokinetics and to avoid the interference of radiolabels with the binding region. For ^18^F labeling, the peptide in anhydrous dimethyl sulfoxide was mixed with dry Cs[^18^F]F/K_2.2.2_ complex and then heated for 15 min at 90°C. The ^18^F-incorporation was 76%. The decay-corrected radiochemical yield of [^18^F]7b was ~14%, and its radiochemical purity and specific activity were >99% and 77 GBq/μmol (2.08 Ci/μmol), respectively, at the end of synthesis. The lipophilicity, expressed as distribution coefficient D (log D_7.4_), was −1.1. The fluorinated peptide had calculated and found molecular weights of 1,376.6 and 1,378.0, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20857927)]

The receptor binding affinity of [^18^F]7b was determined with the use of cell membranes transfected with human GRPR (1). Nonspecific binding was determined with an excess of 10 μM Tyr^4^-BN. The binding affinity (K_i_) of the non-labeled peptide (Ala(SO_3_H)-Ava-Gln-Trp-Ala-Val-NMeGly-His-Sta-Leu-NH_2_) was 0.1 nM, and its half maximal inhibitory concentration (IC_50_) was 0.4 nM. The corresponding K_i_ and IC_50_ values of the [^18^F]7b were 1.43 nM and 0.94 nM, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20857927)]

The biodistribution of [^18^F]7b was studied in nude mice bearing subcutaneous PC-3 human prostate tumors (n = 3 mice/group) (1). [^18^F]7b showed clear tumor targeting. The tumor uptake was 4.67 ± 0.04% injected dose per gram of tissue (ID/g) at 30 min after injection, which increased to 4.88 ± 0.36, 5.40 ± 0.58, and 5.16 ± 1.32% ID/g at 1, 2, and 4 h after injection, respectively. Uptake in the GRPR-rich pancreas was almost 50% ID/g at 1 h after injection. Uptake in the tumor and pancreas was effectively blocked by co-administration of unlabeled BN (83% and 97% specificity, respectively). [^18^F]7b also showed fast blood clearance, leading to favorable tumor/blood ratios of 30.59, 51.77, and 55.03 at 1, 2, and 4 h after injection, respectively. [^18^F]7b was mainly excreted via the hepatobiliary system, resulting in bile/tumor ratios of >20. In vivo defluorination of [^18^F]7b was not evident on the basis of its accumulation in the bone. The % ID/g values in bone were 0.84 ± 0.08, 1.52 ± 0.22, 1.60 ± 0.12, and 1.75 ± 0.23 at 0.5, 1, 2, and 4 h after injection, respectively.

PET imaging with [^18^F]7b was performed in four nude mice bearing subcutaneous PC-3 tumor xenografts (1). The tumors (n = 2 mice) were clearly imaged with [^18^F]7b, which was blocked with unlabeled BN (n = 2 mice). As expected from the biodistribution study, the highest radioactivity was observed in the gallbladder and intestine. The pancreas could not be visualized with PET due to the proximity to the bowel. Postmortem tissue sampling of these mice after PET scanning (107 min after injection) confirmed the data obtained in the biodistribution study. The absolute radioactivity uptake values in the GRPR-rich tissues were 5% ID/g for the tumor and 30% ID/g for the pancreas. The specificity of uptake amounted to 85% and 95% for the tumor and pancreas, respectively. Bone imaging data were not described.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Mu L., Honer M., Becaud J., Martic M., Schubiger P.A., Ametamey S.M., Stellfeld T., Graham K., Borkowski S., Lehmann L., Dinkelborg L., Srinivasan A. (2010). In vitro and in vivo characterization of novel 18F-labeled bombesin analogues for targeting GRPR-positive tumors. Bioconjug Chem.
2 Ischia J., Patel O., Shulkes A., Baldwin G.S. (2009). Gastrin-releasing peptide: different forms, different functions. Biofactors.
3 Weber H.C. (2009). Regulation and signaling of human bombesin receptors and their biological effects. Curr Opin Endocrinol Diabetes Obes.
4 Smith C.J., Volkert W.A., Hoffman T.J. (2003). Gastrin releasing peptide (GRP) receptor targeted radiopharmaceuticals: a concise update. Nucl Med Biol.
5 Schroeder R.P., van Weerden W.M., Bangma C., Krenning E.P., de Jong M. (2009). Peptide receptor imaging of prostate cancer with radiolabelled bombesin analogues. Methods.
6 Smith C.J., Volkert W.A., Hoffman T.J. (2005). Radiolabeled peptide conjugates for targeting of the bombesin receptor superfamily subtypes. Nucl Med Biol.
7 Zhang X., Cai W., Cao F., Schreibmann E., Wu Y., Wu J.C., Xing L., Chen X. (2006). 18F-labeled bombesin analogs for targeting GRP receptor-expressing prostate cancer. J Nucl Med.
8 Ananias H.J., de Jong I.J., Dierckx R.A., van de Wiele C., Helfrich W., Elsinga P.H. (2008). Nuclear imaging of prostate cancer with gastrin-releasing-peptide-receptor targeted radiopharmaceuticals. Curr Pharm Des.
9 Hohne A., Mu L., Honer M., Schubiger P.A., Ametamey S.M., Graham K., Stellfeld T., Borkowski S., Berndorff D., Klar U., Voigtmann U., Cyr J.E., Friebe M., Dinkelborg L., Srinivasan A. (2008). Synthesis, 18F-labeling, and in vitro and in vivo studies of bombesin peptides modified with silicon-based building blocks. Bioconjug Chem.
10 Nock B.A., Nikolopoulou A., Galanis A., Cordopatis P., Waser B., Reubi J.C., Maina T. (2005). Potent bombesin-like peptides for GRP-receptor targeting of tumors with 99mTc: a preclinical study. J Med Chem.
11 Cescato R., Maina T., Nock B., Nikolopoulou A., Charalambidis D., Piccand V., Reubi J.C. (2008). Bombesin receptor antagonists may be preferable to agonists for tumor targeting. J Nucl Med.
12 Becaud J., Mu L., Karramkam M., Schubiger P.A., Ametamey S.M., Graham K., Stellfeld T., Lehmann L., Borkowski S., Berndorff D., Dinkelborg L., Srinivasan A., Smits R., Koksch B. (2009). Direct one-step 18F-labeling of peptides via nucleophilic aromatic substitution. Bioconjug Chem.